# [^18^F]6-(2-Fluoropropyl)-4-methyl-pyridin-2-amine

Chemical name: | [^18^F]6-(2-Fluoropropyl)-4-methyl-pyridin-2-amine
Abbreviated name: | [^18^F]iNOS-9
Synonym:
Agent category: | Compound
Target: | Inducible nitric oxide synthase (iNOS)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS)]

Nitric oxide (NO) is produced as an important mediator in physiological and pathophysiological conditions by three isoforms of NO synthase (NOS): endothelial NOS (eNOS), neuronal NOS (nNOS), and inducible NOS (iNOS) (1, 2). NOSs are highly regulated for specific physiological roles in various tissues and cells. nNOS produces NO in neurons in both the central and peripheral nervous systems as a neurotransmitter and a neuronal modulator for cellular communication. NO is generated in blood vessels by eNOS in endothelial cells for blood pressure regulation. iNOS is induced by various inflammatory stimuli in activated macrophages and other types of cells and plays an important role in immunity and inflammation. iNOS is also essential for host defense against microorganisms and cancer cells.

The basal level of NO is usually very low. In contrast, activated iNOS can generate a large amount of NO over a prolonged period of time during acute and chronic inflammatory diseases (3). iNOS has been found to be overexpressed in a number of tumors compared with normal tissues (4). As a result of the involvement of iNOS in a variety of physiological processes in both normal and diseased states, it is necessary to develop a radiolabeled ligand for noninvasive measurement of iNOS expression. Zhou et al. (5) reported the development of a series of 2-amino-4-methylpyridine analogs as iNOS Inhibitors for positron emission tomography (PET) imaging for iNOS. One of them, [^18^F]6-(2-fluoropropyl)-4-methyl-pyridin-2-amine ([^18^F]iNOS-9), has been tested in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS%20and%20synthesis)]

[^18^F]iNOS-9 was readily synthesized with standard ^18^F-fluorination of the N-BOC–protected mesylate precursor with ([^18^F]KF/Kryptofix2.2.2), followed by acid hydrolysis (5). The radiochemical yield was ~10% (decay-corrected) at the end of purification, and the specific activity was 80 ± 61 GBq/µmol (2.16 ± 1.66 Ci/µmol) at the end of synthesis. Radiochemical purity was >99% as determined with high-performance liquid chromatography. Total synthesis time was 120 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS%20and%20in%20vitro)]

Zhou et al. (5) performed in vitro enzyme inhibition assays for iNOS, eNOS, and nNOS. iNOS-9 exhibited 50% inhibition concentration values of 220 ± 25 nM for iNOS, 1,500 ± 300 nM for eNOS, and 490 ± 80 nM for nNOS. [^18^F]iNOS-9 was 80% and 75% intact in rat blood at 37ºC for 1 h and 2 h, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS%20and%20rodentia)]

[^18^F]iNOS-9 (1.85 MBq (50 μCi)) was injected intravenously into normal and lipopolysaccharide (LPS)-treated mice (n = 4/group) to study the expression of iNOS induced by LPS (5). The organs with the highest accumulation in normal and LPS-treated groups at 60 min after injection were the liver (2.59 and 2.63% injected dose (ID)/g, respectively) and the kidneys (2.20 and 3.95% ID/g, respectively), followed by the lungs (0.31 and 0.73% ID/g), muscle (0.27 and 0.78% ID/g), heart (0.19 and 0.41% ID/g), and brain (0.11 and 0.19% ID/g). The LPS-treated mice exhibited ~30% increase in [^18^F]iNOS-9 accumulation in most of the organs as compared with the control mice. In the lungs (the LPS-targeted organ), LPS-treated mice showed iNOS increases of 30% at 5 min, 60% at 30 min, and 130% at 60 min. Co-administration of the selective iNOS inhibitor 1400W (5 mg/kg) with [^18^F]iNOS-9 blocked the tracer accumulation in the lungs and blood by >32% (P < 0.05) at 60 min after injection. The expression of iNOS was confirmed with Western blot analysis of lung homogenates from the LPS-treated mice. Dynamic [^18^F]iNOS-9 PET scans were performed for 60 min in one normal mouse and one LPS-treated mouse. The lungs in the LPS-treated mouse were clearly visualized at 60 min after injection but the lungs of the normal mouse were not.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+iNOS%20and%20humans)]

No publication is currently available.

## NIH Support

HL13851, CA86307

## References

1 Stuehr D.J. (1999). Mammalian nitric oxide synthases. Biochim Biophys Acta.
2 Nathan C. (1992). Nitric oxide as a secretory product of mammalian cells. Faseb J.
3 Hobbs A.J., Higgs A., Moncada S. (1999). Inhibition of nitric oxide synthase as a potential therapeutic target. Annu Rev Pharmacol Toxicol.
4 Lechner M., Lirk P., Rieder J. (2005). Inducible nitric oxide synthase (iNOS) in tumor biology: the two sides of the same coin. Semin Cancer Biol.
5 Zhou D., Lee H., Rothfuss J.M., Chen D.L., Ponde D.E., Welch M.J., Mach R.H. (2009). Design and synthesis of 2-amino-4-methylpyridine analogues as inhibitors for inducible nitric oxide synthase and in vivo evaluation of [18F]6-(2-fluoropropyl)-4-methyl-pyridin-2-amine as a potential PET tracer for inducible nitric oxide synthase. J Med Chem.